# ^68^Ga-Labeled homoalanine derivatives of 1,4,7,10-tetraazacyclododecane-1,7-diacetic acid and 1,4,7,10-tetraazacyclododecane-1,4,7,-triacetic acid

Chemical name: | ^68^Ga-Labeled homoalanine derivatives of 1,4,7,10-tetraazacyclododecane-1,7-diacetic acid and 1,4,7,10-tetraazacyclododecane-1,4,7,-triacetic acid | [image]
Abbreviated name: | ^68^Ga-23, ^68^Ga-24 | [image]
Synonym: | ^68^Ga-DO2A-homoalanine, ^68^Ga-DO3A-homoalanine | [image]
Agent Category: | Others (amino acid) | [image]
Target: | Amino acid transporters | [image]
Target Category: | Transporters | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | Gallium-68 (^68^Ga) | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of ^68^Ga-23 and ^68^Ga-24 by Shetty et al. (1).

## Background

PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=amino%20acid%20and%20imaging%20and%20amino%20acid%20transporters)]

The ^68^Ga-labeled homoalanine derivatives of 1,4,7,10-tetraazacyclododecane-1,7-diacetic acid (DO2A) and 1,4,7,10-tetraazacyclododecane-1,4,7,-triacetic acid (DO3A), abbreviated as ^68^Ga-23 and ^68^Ga-24, respectively, were synthesized by Shetty et al. for positron emission tomography (PET) of cancer cells (1).

Radiolabeled amino acids represent a diverse class of tracers that target the increased amino acid transport in cancer cells (2, 3). To date, >20 distinct amino acid transporters have been identified in mammalian cells, and these transporters differ in terms of substrate specificity, tissue expression patterns, sodium and other ion dependence, pH sensitivity, and transport mechanism (4, 5). Because of increased demand for amino acids in malignant cells, some transporters have been shown to be overexpressed in different types of tumors, and the process of amino acid transport is relatively fast (2, 6, 7). These features make tumor imaging with amino acid tracers possible within 20 min. Indeed, there is growing evidence that radiolabeled amino acids have the potential to overcome some of the limitations of 2-deoxy-2-[^18^F]fluoro-D-glucose ([^18^F]FDG) in tumor imaging, especially in the imaging of primary and recurrent brain tumors, neuroendocrine tumors, and prostate cancers (2, 3, 8). Different studies also showed that radiotracers that target different amino acid transporters exhibit different imaging properties that may provide unique biological information of tumors (1, 2, 7).

The first group of widely investigated amino acids is the analogs of phenylalanine and tyrosine (2, 3). Because of their bulky neutral side chains, these natural amino acids are the substrates of system L transporters and have been proven to be useful for tumor imaging, particularly for brain tumors. The limitation common to most of the natural amino acids is the susceptibility to in vivo metabolism, which decreases tumor specificity and complicates kinetic analysis. Because none of the natural amino acids contain fluorine or iodine, labeling with fluorine-18 or iodine-123 can alter the biochemistry of the amino acids. These shortcomings associated with natural amino acids can be partially overcome by using non-natural amino acids. Typically, non-natural amino acids are neither metabolized nor readily incorporated into protein in vivo (2, 3, 7). One group of non-natural amino acids is á,á-dialkyl amino acids, which are generated by substituting the á-carbon hydrogen of natural amino acids with a methyl group or other alkyl chains. These amino acids are primarily the substrates of system A transporters. The second group is alicyclic amino acids, which are á,á-dialkyl amino acids with side chains bonded covalently to each other to form a cyclic ring. These amino acids are the substrates of system L transporters. The third group is non-natural proline derivatives, which exhibit different transport selectivity. One challenge in developing amino acid radiotracers is to overcome the low selectivity and the decreased recognition after radiolabeling to specific transporters (1-3). Another challenge is the low uptake of amino acid agents in tumors, which leads to less sensitivity for tumor detection than with [^18^F]FDG (8).

Shetty et al. synthesized a group of ^68^Ga-labeled alanine and lysine derivatives of 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA), 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA), DO2A, and DO3A (1, 7). The four bifunctional chelating agents have similar sizes, but they differ in the net charges because of the different numbers of pendent carboxylate arms. The amino acids have been conjugated to one of the carboxylate arms, and the nitrogen atoms in the heterocyclic ring are presumed to coordinate with metals to form chelates. Biodistribution studies and PET imaging indicate the structure–activity relationship of the amino acid derivatives, and the selective uptakes of these compounds by different cancer tissues might provide an insight on the different modes of amino acid uptake by cancer cells (1, 7).

This chapter summarizes the data obtained with ^68^Ga-labeled homoalanine derivatives: ^68^Ga-23 (^68^Ga-DO2A-homoalanine) and ^68^Ga-24 (^68^Ga-DO3A-homoalanine). These homoalanine derivatives were comparatively analyzed with the corresponding alanine derivatives (^68^Ga-21 and ^68^Ga-22, respectively) (1).

### Related Resource Links:

Amino acid transporter-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amino+acid+transporter+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Amino acid transporter articles in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/?term=amino+acid+transporter)

Amino acid transporter related clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amino+acid+transporter)

Amino acid transporter related bioassays in PubChem BioAssay (http://www.ncbi.nlm.nih.gov/pcassay/?term=amino+acid+transporter)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21055619)]

Shetty et al. synthesized the homoalanine derivatives, DO2A-homoalanine (compound 23) and DO3A-homoalanine (compound 24), by reacting bromohomoalanine with the compounds 1,4,7,10-tetracyclododecene-1,7-bis(tert-butyl acetate) and 1,4,7,10-tetracyclododecene-1,4,7-tris(tert-butyl acetate), respectively (1). The final homoalanine derivatives were obtained after catalytic hydrogenation and subsequent acid hydrolysis.

Radiolabeling of the derivatives with ^68^Ga was carried out at pH 3–4. The labeled reaction mixture was passed through a cartridge to remove the free ^68^Ga^3+^. The labeled agents were analyzed with radiographic thin-layer chromatography. The labeling efficiencies were >97% for both ^68^Ga-23 (^68^Ga-DO2A-homoalanine) and ^68^Ga-24 (^68^Ga-DO3A-homoalanine). No free ^68^Ga was found after purification. DOTA without an amino acid residue was labeled with ^68^Ga under the same conditions (^68^Ga-DOTA) and was used as the control for in vitro cell uptake study. The specific activities and stabilities of ^68^Ga-23, ^68^Ga-24, and ^68^Ga-DOTA were not reported (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21055619)]

Cell uptake assays were performed after incubation of Hep3B (human hepatoma) and U87MG (human glioma) cells with 10 ìCi (0.37 MBq) of each agent at 37°C for various times (1). Both ^68^Ga-23 and ^68^Ga-24 exhibited greater uptakes than the control ^68^Ga-DOTA. ^68^Ga-23 showed a higher uptake than ^68^Ga-24 in both cell lines.

Comparative analysis was performed for the cell uptake between alanine and homoalanine derivatives (1). The results showed that all agents (^68^Ga-21 to ^68^Ga-24) exhibited higher uptake than ^68^Ga-DOTA in both cell lines. ^68^Ga-22 had the highest uptake in U87MG cells, whereas ^68^Ga-23 had the highest uptake in Hep3B cells. These results may represent specific uptakes of the amino acid derivatives by cancer cells due to different expressions of various amino acid transporters on cell surfaces. Shetty et al. did not perform blocking experiments, considering that many amino acid derivatives can be transported simultaneously by several different types of transporters and the cell uptake cannot be completely blocked by a single inhibitor (1). No further definition of the uptake mechanism in vitro was included.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21055619)]

The biodistribution patterns of ^68^Ga-23 and ^68^Ga-24 were investigated at 10, 30, 60, and 120 min after tail vein injection of each agent (10 ìCi (0.37 MBq)) in mice bearing CT-26 colon cancer xenografts (n = 3–4 mice/time point for each agent) (1). The initial tumor uptakes at 10 min after injection was 2.68% and 2.80% injected dose per gram of tissue (ID/g) for ^68^Ga-23 and ^68^Ga-24, respectively, which rapidly decreased to 0.80% for ^68^Ga-23 and 0.99% for ^68^Ga-24 at 60 min and to 0.55% for ^68^Ga-23 and 0.57% for ^68^Ga-24 at 120 min after injection. The tumor/muscle and tumor/blood ratios peaked at 120 min after injection. The tumor/muscle ratios for ^68^Ga-23 and ^68^Ga-24 were 4.53 and 7.42 at 120 min, respectively. The tumor/blood ratios for ^68^Ga-23 and ^68^Ga-24 were 1.36 and 3.51 at 120 min, respectively. PET imaging was performed at 30 min after tail vein injection (0.37 MBq (0.01 mCi)) and showed that ^68^Ga-23 had higher tumor uptake than ^68^Ga-24.

Comparative analysis was also performed for the biodistribution and PET imaging data between alanine and homoalanine derivatives (1). Comparison for the biodistribution showed that all of the alanine and homoalanine derivatives (^68^Ga-21 to ^68^Ga-24) presented high kidney uptake and low liver and intestine uptake, indicating that the major excretion route of these agents is the kidney. The tumor uptake of alanine derivatives (^68^Ga-21 and ^68^Ga-22) was higher than that of homoalanine derivatives (^68^Ga-23 and ^68^Ga-24) at both 30 min and 60 min. However, homoalanine derivatives had higher tumor/nontumor ratios than alanine derivatives at all investigated time points.

Similarly, high kidney and bladder activities were observed for all agents in PET imaging. The alanine derivatives showed higher tumor uptakes than the homoalanine derivatives. The SUV for all agents was lower than that of [^18^F]FDG, which might be the result of slow uptake by cancer tissues and rapid excretion through the kidneys. However, tumor/nontumor SUV ratios were high enough to obtain tumor images. ^68^Ga-24 showed the highest tumor/nontumor SUV ratio (3.9 ± 0.3), followed by ^68^Ga-21 (3.1 ± 0.2), ^68^Ga-22 (2.8 ± 0.2), and ^68^Ga-23 (2.3 ± 0.2). No further experiments on the possible mechanism in vivo were included.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Shetty D., Jeong J.M., Ju C.H., Lee Y.S., Jeong S.Y., Choi J.Y., Yang B.Y., Lee D.S., Chung J.K., Lee M.C. (2010). Synthesis of novel 68Ga-labeled amino acid derivatives for positron emission tomography of cancer cells. Nucl Med Biol.
2 McConathy, J., W. Yu, N. Jarkas, W. Seo, D.M. Schuster, and M.M. Goodman, Radiohalogenated nonnatural amino acids as PET and SPECT tumor imaging agents. Med Res Rev, 2011
3 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
4 Ganapathy V., Thangaraju M., Prasad P.D. (2009). Nutrient transporters in cancer: relevance to Warburg hypothesis and beyond. Pharmacol Ther.
5 Goberdhan D.C. (2010). Intracellular amino acid sensing and mTORC1-regulated growth: new ways to block an old target?. Curr Opin Investig Drugs.
6 Fuchs B.C., Bode B.P. (2005). Amino acid transporters ASCT2 and LAT1 in cancer: partners in crime?. Semin Cancer Biol.
7 Shetty D., Jeong J.M., Ju C.H., Kim Y.J., Lee J.Y., Lee Y.S., Lee D.S., Chung J.K., Lee M.C. (2010). Synthesis and evaluation of macrocyclic amino acid derivatives for tumor imaging by gallium-68 positron emission tomography. Bioorg Med Chem.
8 la Fougere C., Suchorska B., Bartenstein P., Kreth F.W., Tonn J.C. (2011). Molecular imaging of gliomas with PET: Opportunities and limitations. Neuro Oncol.